# ^99m^Tc-Labeled peptide derivative of folic acid

Chemical name: | ^99m^Tc-Labeled peptide derivative of folic acid
Abbreviated name: | ^99m^Tc-EC20
Synonym:
Agent Category: | Compound
Target: | Folate receptor (Folate binding protein)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Structure of ^99m^Tc-EC20 according to Leamon et. al. (1)

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=folate+receptor+imaging)

Folic acid (FA; folate) belongs to the B group of vitamins, and its activity is mediated through the membrane-bound folate receptor (FR; also known as the folate-binding protein), which has two isoforms (α and β). A third constitutively secreted form of the receptor (γ) has also been identified in some hematopoietic cells (2). The α and β isoforms of FR show a high affinity for FA and exhibited restricted expression in certain tissues. FR-α is found in the lungs, glandular tissue, and choroid plexus of the brain. A functional β form is present only in activated monocytes and macrophages, although it is also borne by mature neutrophils and CD34^+^ cells (as an inactive form) (2). Low amounts of FR-α are expressed in normal tissue, but it was shown to be overexpressed in several cancerous tumors such as those of the breast, colon, head and neck, kidneys, and lungs (3). In addition, overexpression of the FR in tumors indicates a poor prognosis for the patient (4, 5). Therefore, the FR has been targeted in clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor&map=ES) for the detection, diagnosis, and treatment of various cancers. Several folate-based imaging agents that use techniques such as magnetic resonance imaging, optical imaging, computed tomography, positron emission tomography, and single-photon emission tomography (SPECT) have been developed and evaluated for the noninvasive detection of malignant tumors that had excessive expression of FR (3). However, except for the SPECT-based agents, all imaging agents had limited use and were determined to be unsuitable for detection of tumors overexpressing the FR as detailed by Sega et al. (3).

An indium (^111^In)-labeled folate-based SPECT agent with a good tumor specificity was developed earlier and evaluated in clinical trials, but the nuclide is expensive to produce, has a high γ energy emission (171 and 245 keV), and has a long half-life (~68 h) (3), and the detection of recurrent cancer with this agent is difficult (6). To overcome the problems associated with the use of ^111^In, some investigators developed and evaluated the use of technetium (^99m^Tc)-labeled FR imaging agents because this nuclide has a low energy emission (140 keV), has a short half-life (~6 h), is inexpensive to produce, and, compared with ^111^In, produces high-quality images (1, 7-11). Among the different ^99m^Tc-labeled FR imaging agents, only the peptide-based, folate-derived compound ^99m^Tc-EC20 (folic acid-pteroic acid (Pte)-D-Glu-β-L-diaminopropionic acid(βDpr)-Asp-Cys) has been evaluated in a mouse model (1, 12, 13), and more recently it was used for an exploratory study in humans to detect the presence of FR-positive tumors (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+tc+EC20)]

The synthesis of EC20 and its labeling with ^99m^Tc was described by Leamon et al. (1). The synthesized EC20 was purified with high-performance liquid chromatography (HPLC) and analyzed with nuclear magnetic resonance imaging and electrospray-mass spectrometry. Kits containing a sterile, nonpyrogenic mixture of purified EC20, sodium α-D glucoheptonate, tin chloride, and sodium hydroxide or hydrochloric acid (to maintain a pH of 6.8 ± 0.2) were subsequently prepared in reagent vials for lyophilization. The lyophilized preparation was sealed under argon and stored at -20°C until use. The shelf-life of the lyophilized kit under these storage conditions was reported to be >2 years (1).

The labeling of EC20 was done by injecting ^99m^Tc-pertechnetate into the EC20 kit vial and by heating it in a boiling water bath for ~18 min (1). The labeled product was allowed to cool for at least 15 min at room temperature and used within 6 h of preparation. From an HPLC analysis of the labeled product, the investigators concluded that it had a purity of >95% but probably contained a diastereomeric mixture of the labeled product (1). Radiochemical purity of the reconstituted labeled compound was reported to be >90% for up to 24 h when stored at room temperature. The specific activity of ^99m^TC-EC20 was not reported. Chelation of ^99m^Tc to EC20 is shown in the chemical structure of the compound as suggested by Leamon et. al. (1). Other ^99m^Tc-labeled analogs of EC20 (^99m^TC-EC14 and ^99m^TC-EC28; for details regarding their respective structures, see Leamon et al. (1)) and ^111^In-diethylenetriamine pentaacetic acid (DTPA)-folate, a previously used radiopharmaceutical (15), were also prepared for some studies by the investigators (1), but their radiochemical purity, specific activity, and stability were not reported.

In another study, an all-D isomer of EC20, designated EC53, was synthesized, purified, lyophilized, and labeled with ^99m^Tc as detailed above (12). The radiochemical purity of ^99m^Tc-EC53 was >90%. The stability of reconstituted EC53 was reported to be the same as that of EC20 for at least 24 h at room temperature. Specific activity of the labeled compound was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+tc+EC20+in+vitro)]

An analysis of ^99m^Tc-EC20 exposed to rat or human serum showed that ~70% of the radiochemical was bound to a >30-kDa serum protein in both sera (1). However, the investigators concluded that this did not affect biodistribution of the radiocompound because it was detected in all the FR-positive tissue (see below for details).

The FR binding affinity of ^99m^Tc-EC20 in KB cells (http://atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-17&Template=cellBiology) was reported to be 1.1 nM (1), and the binding was completely blocked in the presence of excess (100 nM) folic acid. Compared with folic acid, the relative affinity (RA; defined as the inverse molar ratio of compound required to displace 50% of ^3^H-folic acid bound to FR on KB cells; the RA of folic acid was taken to be 1.0) values of ^99m^Tc-EC20 and DTPA-folate was determined to be 0.92 ± 0.23 and 0.87 ± 0.16, respectively. In the same study, the diastereoisomers of ^99m^Tc-EC20 (with either a syn or an anti configuration of the ^99m^Tc-oxygen bond in the DAP-Asp-Cys chelating ring of EC20) were reported to have an RA of 1.42 ± 0.36 and 1.37 ± 0.23, respectively. In another study, EC53, an all-D isomeric molecule of EC20, was shown to have an RA of 0.23 (12).

Reddy et al. investigated the effect of FR expression level on the uptake of ^99m^Tc-EC20 in tumor cells (12). Tumors derived from 4T1 (expressing 1.5 pmol FR/mg protein), M109 (expressing 22.9 pmol FR/mg protein), and 4T1-pico (expressing 7.2 pmol FR/mg protein) cells were harvested from mice exposed to ^99m^Tc-EC20. The amount of radioactivity associated with cell membranes of the respective tumors was determined and reported to be proportional to the expression of FR by the various cells (2.6 ± 0.7, 8.7 ± 2.3, and 15.53 ± 1.90 percent injected dose/gram tissue (% ID/g) for the 4T1, 4T1-pico, and the M109 tumor cells, respectively). In addition, when the radiotracers were co-injected with 100-fold excess unlabeled folic acid, <1% ID/g accumulation of radioactivity was observed in the three tumor types, indicating that the uptake of label in these tumors was primarily due to presence of the FRs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+tc+EC20+rodentia)]

To investigate the biodistribution of ^99m^Tc-EC14 (compared to EC20 an additional D-Glu residue is present in the EC14 peptide sequence), ^99m^Tc-EC20, ^99m^Tc-EC28 (negative control; compared to EC20 the sequence of the peptide in EC28 is Pte-D-Glu-D-Glu-βDpr-Asp-Cys), and ^111^In-DTPA-folate (positive control), BALB/c mice (n = 3 animals per cohort) bearing M109 cell tumors were injected with the radiotracers through the lateral tail vein and euthanized 4 h later (1). The major tissues, including tumors, were removed from the animals, weighed, and counted for accumulated radioactivity. Compared with ^99m^Tc-EC14, ^99m^Tc-EC20, and ^111^In-DTPA-folate, only a small amount of ^99m^Tc-EC28 accumulated in the tumors and kidney (this organ contains high levels of FR). The other three folate-containing radiochemicals accumulated mainly in the tumors and the kidneys of the animals. The kidneys showed a higher uptake of the label compared to the tumors. The accumulation of ^99m^Tc-EC20 and ^111^In-DTPA-folate in the tumors was similar (17.2 ± 1.02 and 19.3 ± 5.86% ID/g, respectively), and for ^99m^Tc-EC14 it was 9.83 ± 2.77% ID/g. When the radiolabeled folate compounds were injected along with a 100-fold excess of unlabeled folic acid, a significantly reduced uptake (P value not reported) of the respective labeled compounds in the tumors and kidneys was reported. This indicated that cell binding of the radiolabeled folate compounds was specific for FR.

Mice bearing M109 cell tumors underwent whole-body gamma planar imaging 4 h after treatment with ^99m^Tc-EC20. The imaging showed that the radioactivity had accumulated primarily in the tumors and kidneys of the animals, which confirmed observations made during the biodistribution studies (1). No blocking studies were reported.

Reddy et al. studied the biodistribution of ^99m^Tc-EC20 and ^99m^Tc-EC53 in BALB/c mice (n = 3 animals/labeled compound) bearing M109 cell tumors (12). The animals were injected with the respective radiochemicals and euthanized 4 h later, and the radioactivity accumulated in the various organs was measured as described elsewhere (1). Although both tracers accumulated mainly in the tumors and the kidneys, the level of radioactivity in these tissues for animals treated with ^99m^Tc-EC53 was ~33.0% less than that observed with ^99m^Tc-EC20. In addition, tumor size, tumor location (subcutaneous or intraperitoneal), and route of radiotracer administration were reported to have no effect on uptake of the radiochemicals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+tc+EC20+Non-Primate+Mammals)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+tc+EC20+Non+Human+Primates)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+tc+EC20+imaging+in+Humans)]

The accumulation of ^99m^Tc-EC20 in solid tumors and its correlation with FR expression, as determined with immunohistochemical (IHC) analysis, was investigated in a preliminary study of 154 cancer patients (14). Among these patients, 77% had a diagnosis of renal cell carcinoma and the remaining patients had a variety of other solid tumors. Gamma planar imaging was performed 1–2 h after treatment with ^99m^Tc-EC20, followed by single-photon emission computed tomography of the index lesion regions. Data obtained with ^99m^Tc-EC20 correlated with the IHC analysis of tissue available after surgery or from biopsies to detect the expression of FR-α. The accumulation of radioactivity in tumors was reported in 68% of the patients, and 67% of the tumors expressed FR-α. The two methods had an overall agreement of 61% (k = 0.096; 95% confidence interval = -0.085–0.277). There was 72% and 38% agreement of the positive and negative results, respectively, between the two methods.

From these results the investigators concluded that ^99m^Tc-EC20 was safe and well tolerated by humans. The radiochemical could probably be used for a noninvasive procedure to select patients who could potentially benefit from FR-targeted therapy (14).

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## References

1 Leamon C.P., Parker M.A., Vlahov I.R., Xu L.C., Reddy J.A., Vetzel M., Douglas N. (2002). Synthesis and biological evaluation of EC20: a new folate-derived, (99m)Tc-based radiopharmaceutical. Bioconjug Chem.
2 Leamon C.P. (2008). Folate-targeted drug strategies for the treatment of cancer. Curr Opin Investig Drugs.
3 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.
4 Hartmann L.C., Keeney G.L., Lingle W.L., Christianson T.J., Varghese B., Hillman D., Oberg A.L., Low P.S. (2007). Folate receptor overexpression is associated with poor outcome in breast cancer. Int J Cancer.
5 Allard J.E., Risinger J.I., Morrison C., Young G., Rose G.S., Fowler J., Berchuck A., Maxwell G.L. (2007). Overexpression of folate binding protein is associated with shortened progression-free survival in uterine adenocarcinomas. Gynecol Oncol.
6 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
7 Guo W., Hinkle G.H., Lee R.J. (1999). 99mTc-HYNIC-folate: a novel receptor-based targeted radiopharmaceutical for tumor imaging. J Nucl Med.
8 Ilgan S., Yang D.J., Higuchi T., Zareneyrizi F., Bayhan H., Yu D., Kim E.E., Podoloff D.A. (1998). 99mTc-ethylenedicysteine-folate: a new tumor imaging agent. Synthesis, labeling and evaluation in animals. Cancer Biother Radiopharm.
9 Mathias C.J., Hubers D., Low P.S., Green M.A. (2000). Synthesis of [(99m)Tc]DTPA-folate and its evaluation as a folate-receptor-targeted radiopharmaceutical. Bioconjug Chem.
10 Panwar P., Shrivastava V., Tandon V., Mishra P., Chuttani K., Sharma R.K., Chandra R., Mishra A.K. (2004). 99mTc-Tetraethylenepentamine-Folate--a new 99mTc-based folate derivative for the detection of folate receptor positive tumors: synthesis and biological evaluation. Cancer Biol Ther.
11 Trump D.P., Mathias C.J., Yang Z., Low P.S., Marmion M., Green M.A. (2002). Synthesis and evaluation of 99mTc(CO)(3)-DTPA-folate as a folate-receptor-targeted radiopharmaceutical. Nucl Med Biol.
12 Reddy J.A., Xu L.C., Parker N., Vetzel M., Leamon C.P. (2004). Preclinical evaluation of (99m)Tc-EC20 for imaging folate receptor-positive tumors. J Nucl Med.
13 Turk M.J., Breur G.J., Widmer W.R., Paulos C.M., Xu L.C., Grote L.A., Low P.S. (2002). Folate-targeted imaging of activated macrophages in rats with adjuvant-induced arthritis. Arthritis Rheum.
14 Fisher R.E., Siegel B.A., Edell S.L., Oyesiku N.M., Morgenstern D.E., Messmann R.A., Amato R.J. (2008). Exploratory study of 99mTc-EC20 imaging for identifying patients with folate receptor-positive solid tumors. J Nucl Med.
15 Mathias C.J., Wang S., Waters D.J., Turek J.J., Low P.S., Green M.A. (1998). Indium-111-DTPA-folate as a potential folate-receptor-targeted radiopharmaceutical. J Nucl Med.